# ^111^In-Labeled anti-epidermal growth factor receptor Affibody PEP09239

Chemical name: | ^111^In-Labeled anti-epidermal growth factor receptor Affibody PEP09239
Abbreviated name: | [^111^In]PEP09239
Synonym: | MUT-DS
Agent Category: | Anitbody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20affibody&cmd=DetailsSearch)]

The human epidermal growth factor receptor-2 (HER2, ErbB2) modulates its activity through a tyrosine kinase (TK) signaling pathway and is involved in the development of a variety of cancers (1, 2). Overexpression or amplification of the HER2 gene is known to occur in many cancer types (e.g., ~20% of breast cancer) and predicts a poor prognosis for the patient. Invasive methods, such as biopsies, in conjunction with immunohistochemistry and an in situ fluorescence hybridization kit (PathVysion (http://www.abbottmolecular.com/us/products/oncology/fish/breast-cancer-pathvysion-her2.html)) approved by the United States Food and Drug Administration are used to assess the HER2 status of the primary and metastasized neoplastic tumors; however, because of sampling bias and tumor heterogeneity, results obtained with these procedures are not reliable (2). In the clinic, ^18^F-labeled fluorodeoxyglucose ([^18^F]-FDG) is commonly used with positron emission tomography (PET) to detect and determine the tumor burden of a patient, but this imaging agent does not distinguish between benign and malignant lesions, cannot differentiate tumors that overexpress HER2 from those that have a low or no expression of the receptor, and often identifies inflammation as a false-positive neoplasm (1).

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained via chemical synthesis or produced in bacteria with the use of recombinant DNA technology (3). The Affibody scaffold consists of 3-helix peptide chains: helix chains 1 and 2 are composed of 13 randomized amino acids and contain the receptor-binding moieties of the Affibody (4), and the third helix chain functions as a stabilizer of the Affibody molecule (5). Affibody molecules have high affinity and specificity of binding to the targeted molecule and are considered to be extremely suitable for the noninvasive imaging of solid tumors (6). The radionuclide-labeled Affibody Z_HER2:342_ (and its derivatives), directed against the HER2 (Z_HER2:342_K_d_ = 22 pM for HER2), has been used successfully with molecular imaging techniques to screen for breast cancer patients who are likely to benefit most from treatment with trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2) (a monoclonal antibody that targets HER2) or lapatinib (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=63319b01-cad6-4d0a-c39b-938fa951a808) (a small-molecule drug that inhibits the TK activity of the HER2 signaling pathway) (6, 7).

To further improve the imaging properties of radiolabeled Affibodies, it was hypothesized that reducing the size of the molecule is likely to facilitate rapid clearance of the tracer from circulation, high penetration into solid tumors, ameliorate the uptake of label in nontargeted organs (such as the liver), and generate increased tumor/background ratios compared with the 3-helix molecule (8). To test the hypothesis, the stabilizing helix chain was removed from the 3-helix Z_HER2:342_ molecule, and the 2-helix Affibody (MUT-DS; ~4.6 kDa) was determined to have a binding affinity of 5 nM for HER2 (8). In another study, MUT-DS was conjugated with DOTA, a metal chelator, labeled with ^68^Ga ([^68^Ga]-DOTA-MUT-DS), and evaluated for the detection of human ovarian carcinoma SKOV3 cell xenograft tumors (these cells overexpress HER2) in nude mice (9). Although [^68^Ga]-DOTA-MUT-DS was rapidly cleared from circulation and had a high binding specificity for the tumors, it was observed that the uptake of radioactivity in the lesions was considerably lower (4.12 ± 0.83% injected dose per gram tissue (ID/g) at 2 h postinjection (p.i.)) (9) than the accumulation of label observed in the SKOV3 cell tumors with a similarly labeled HER2-binding 3-helix Affibody ([^68^Ga]-ABY-002; 12.4 ± 3.8% at 2 h p.i.) (10). This indicated that there was no particular advantage in using a smaller Affibody compared with the larger parent 3-helix molecule. In addition, the comparison between the two Affibody types may be inaccurate for two reasons. First, the data that were compared were obtained from two separate studies in which the two SKOV3 cell subclones used to generate the tumors in the mice may not have produced lesions of the same size. Second, the same amounts of HER2 may not have been expressed in the neoplasms (4). Therefore, to ascertain the similarities or dissimilarities between MUT-DS and ABY-002 Affibodies, it was necessary to investigate the biological characteristics of the two entities simultaneously with the use of identical handling techniques and to perform similar in vitro and in vivo studies simultaneously with the two Affibodies (4).

Rosik et al. compared the receptor targeting and biodistribution characteristics of ^111^In-labeled MUT-DS ( [^111^In]PEP09239) and ^111^In-labeled ABY-002 ([^111^In]ABY-002) in a side-by-side study of mice bearing xenograft tumors generated with SKOV3 cells (these cells express ~1.2 × 10^6^ HER2 receptor/cell) and human colorectal LS174T cells (these cells express low levels of HER2; ~3.9 × 10^4^ receptors/cell), respectively (4).

### Related Resource Links

Anti-HER2 affibodies in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-HER2+affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=HER2) related to HER2

Other EGFR-imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books?cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log$=booksrch&bname=micad)

EGFR (human) ligands in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch)

Human EGFR in Online Mendelian Inheritance in Man database (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR))

Information on human EGFR gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein) (Gene ID: 1956)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding human EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-PEP09239%20synthesis&cmd=DetailsSearch)]

Synthetic DOTA-ABY-002, synthesized with the Fmoc procedure, was obtained from a commercial source (4). PEP09239 was also synthesized with the Fmoc technique on an automated peptide synthesizer, and the identity of this Affibody was confirmed with reverse-phase high-performance liquid chromatography (HPLC) and HPLC-mass spectrometry (4). PEP09239 was subsequently conjugated with DOTA and purified with HPLC. The purity of the DOTA-PEP09239 conjugate was reported to be >97% as determined with HPLC (4).

The labeling of DOTA-PEP09239 with ^111^In is described elsewhere (4). The radiochemical yield (RCY) of [^111^In]PEP09239 was 99.4 ± 0.5%, with a specific activity of 5.1 GBq/μmol (137.83 mCi/μmol). The ^111^In-labeled Affibody was used in the various studies without further purification.

DOTA-ABY-002 was labeled with ^111^In as described by Orlova et al. (11). The RCY, radiochemical purity, and SA of [^111^In]ABY-002 were not reported (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEP09239%20in%20vitro%20studies&cmd=DetailsSearch)]

The stability of [^111^In]PEP09239 was evaluated by exposing the ^111^In-labeled Affibody to 1,000-fold molar excess ethylenediamine tetracetic acid (EDTA) for 4 h at room temperature (4). Control samples were incubated in phosphate-buffered saline under the same conditions. At the end of the incubation, 96.1 ± 0.5% of [^111^In]PEP09239 exposed to EDTA was intact (compared with 98.5 ± 0.7% of the control) as determined with radio-thin-layer chromatography.

The binding kinetics of PEP09239 and ABY-002 were determined with surface plasmon resonance techniques, with the extracellular domain of HER2 as the target on the sensor chip (4). The dissociation constants of PEP09239 and ABY-002 were 2.1 nM and 78 pM, respectively. The K_a_ and K_d_ values for PEP09239 were 6.0 × 10^5^ M−^1^s−^1^ and 1.3 × 10−^3^ s−^1^, respectively, and for ABY-002 these values were 4.0 × 10^6^ M−^1^s−^1^ and 2.6 × 10−^4^ s−^1^, respectively.

The receptor binding specificity of [^111^In]PEP09239 was determined by exposing SKOV3 cells and LS174T cells to the labeled Affibody (10 nM) for 1 h at 37°C as described by Rosik et al. (4). Approximately 30% and 1.75% of added radioactivity was bound to the SKOV3 cells and the LS174T cells, respectively. Prior exposure of the SKOV3 cells to either non-radiolabeled PEP09239 or non-radiolabeled ABY-002 reduced the binding to ~1% of total added radioactivity. Similarly, blocking the HER2 receptors on the LS174T cells with non-radiolabeled PEP09239 or non-radiolabeled ABY-002 reduced the binding of [^111^In]PEP09239 to ~0.75% of total added radioactivity. These studies indicated that [^111^In]PEP09239 had a high binding specificity for the HER2 receptor.

In another study, SKOV3 cells were loaded with [^111^In]PEP09239 at 4°C for 1 h and then transferred to growth medium containing no labeled Affibody at 37°C. Subsequently, the amount of radioactivity bound to and internalized by the cells at different time points was determined (4). At 8 h after the transfer, 63 ± 1% of the label (compared with 100% at 0 h) was associated with the cells and remained relatively constant thereafter for up to 24 h. Internalization of the label from [^111^In]PEP09239 was slow and reached up to 21.1 ± 0.5% of the initial value at 24 h after transfer to medium containing no radioactivity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEP09239%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]PEP09239 and [^111^In]ABY-002 was compared in normal Naval Medical Research Institute mice (4). The animals (n = 4 mice/time point) were injected with 30 kBq (0.81 μCi) [^111^In]PEP09239 or [^111^In]ABY-002 through the tail vein and euthanized at predetermined time points ranging from 1 h p.i. to 24 h p.i. All organs of interest were removed from the animals, and the amount of radioactivity accumulated in the various tissues was determined. Data obtained from this study are shown in Table 1. A rapid clearance of radioactivity was observed from the blood and other tissues with both labeled Affibodies; the label from [^111^In]PEP09239 was cleared from all the tissues more rapidly than the label from [^111^In]ABY-002. A high reabsorption of tracer was observed in the kidneys with both tracers, a characteristic common to all HER2-binding Affibodies.

The biodistribution of [^111^In]PEP09239 and [^111^In]ABY-002 was also investigated in outbred BALB/c nu/nu mice bearing SKOV-3 cell and LS714T cell xenograft tumors on the right hind legs (4). The animals (n = 4 mice/time point) were injected with 30 kBq (0.14 nmol) [^111^In]PEP09239 or [^111^In]ABY-002 in 100 μl PBS through the tail vein. The rodents were euthanized at 1 h p.i. and 4 h p.i. to determine the amount of radioactivity accumulated in the various tissues. At 1 h p.i., the uptake of label from [^111^In]ABY-002 in the SKOV3 cell tumors (high expression of HER2) was 1.7-fold higher (17.8 ± 0.4% ID/g) than the uptake from [^111^In]PEP09239 (10.6 ± 0.4% ID/g; P < 0.005), and almost no change in uptake of the tracers was observed for up to 4 h p.i. With the LS174T tumors (low expression of HER2), the accumulation of radioactivity with [^111^In]ABY-002 (8.6 ± 4.0% ID/g) was ~3-fold higher than with [^111^In]PEP09239 (2.9 ± 0.6% ID/g) at 1 h p.i. At 4 h p.i., the uptake of label from [^111^In]ABY-002 in the LS174T cell tumors was ~8-fold higher than with [^111^In]PEP09239 (because with [^111^In]PEP09239 the amount of radioactivity in the LS174T cell tumors was observed to decrease by 4 h p.i.).

To ascertain the HER2 binding specificity of [^111^In]PEP09239, mice bearing SKOV3 cell tumors and LS174T cell tumors (n = 4 animals/tumor type) were subcutaneously pretreated with 115.4 nmol (for SKOV3 cell tumors) or 76.9 nmol (for LS174T cell tumors) non-radioactive Z_HER2:342_; 40 min later, the animals were intravenously injected with the labeled 2-helix Affibody (4). Pretreatment of the animals with excess non-labeled Z_HER2:342_ resulted in a significantly lower (P < 0.05) accumulation of radioactivity in both the tumor types; however, no reduced uptake of tracer was apparent in any other organs. These results indicated that [^111^In]PEP09239 had a high binding specificity for HER2.

For PET imaging studies (to confirm the biodistribution data), mice bearing SKOV3 cell tumors and LS174T cell tumors were injected with 0.6 MBq (16.2 μCi) [^111^In]PEP09239 or [^111^In]ABY-002, and the animals were euthanized at 4 h p.i (4). The urinary bladders of the animals were removed immediately before imaging, and gamma planar images of the rodents were acquired for 60 min. From the images it was clear that both tumor types were clearly visible only in rodents injected with [^111^In]ABY-002, but the amount or tracer accumulated in the LS174T cell lesions was lower than that in the SKOV3 cell tumors. With [^111^In]PEP09239, only the SKOV3 cell tumors were clearly visible, and the LS174T cell lesions were only faintly visible in the animals.

From these studies, the investigators concluded that radioactivity from the 2-helix [^111^In]PEP09239 Affibody was cleared rapidly from circulation and normal tissues of the rodents compared with the label from [^111^In]ABY-002 (4). In addition, although the uptake of label from [^111^In]PEP09239 in the neoplastic lesions with a high expression of HER2 was lower than with [^111^In]ABY-002, the tumor/blood ratio with the former labeled Affibody was higher than that with the latter labeled Affibody (4). However, [^111^In]ABY-002 appeared to be superior to [^111^In]PEP09239 for the visualization of tumors that have a low expression of HER2 (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEP09239%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEP09239%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEP09239%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kramer-Marek G., Bernardo M., Kiesewetter D.O., Bagci U., Kuban M., Omer A., Zielinski R., Seidel J., Choyke P., Capala J. (2012). PET of HER2-Positive Pulmonary Metastases with 18F-ZHER2:342 Affibody in a Murine Model of Breast Cancer: Comparison with 18F-FDG. J Nucl Med.
2 Kramer-Marek G., Gijsen M., Kiesewetter D.O., Bennett R., Roxanis I., Zielinski R., Kong A., Capala J. (2012). Potential of PET to predict the response to trastuzumab treatment in an ErbB2-positive human xenograft tumor model. J Nucl Med.
3 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
4 Rosik D., Orlova A., Malmberg J., Altai M., Varasteh Z., Sandstrom M., Karlstrom A.E., Tolmachev V. (2012). Direct comparison of 111In-labelled two-helix and three-helix Affibody molecules for in vivo molecular imaging. Eur J Nucl Med Mol Imaging.
5 Honarvar H., Jokilaakso N., Andersson K., Malmberg J., Rosik D., Orlova A., Karlstrom A.E., Tolmachev V., Jarver P. (2013). Evaluation of backbone-cyclized HER2-binding 2-helix Affibody molecule for In Vivo molecular imaging. Nucl Med Biol.
6 Ahlgren S., Tolmachev V. (2010). Radionuclide molecular imaging using Affibody molecules. Curr Pharm Biotechnol.
7 Baum R.P., Prasad V., Muller D., Schuchardt C., Orlova A., Wennborg A., Tolmachev V., Feldwisch J. (2010). Molecular imaging of HER2-expressing malignant tumors in breast cancer patients using synthetic 111In- or 68Ga-labeled affibody molecules. J Nucl Med.
8 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
9 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
10 Tolmachev V., Velikyan I., Sandstrom M., Orlova A. (2010). A HER2-binding Affibody molecule labelled with 68Ga for PET imaging: direct in vivo comparison with the 111In-labelled analogue. Eur J Nucl Med Mol Imaging.
11 Orlova A., Tolmachev V., Pehrson R., Lindborg M., Tran T., Sandstrom M., Nilsson F.Y., Wennborg A., Abrahmsen L., Feldwisch J. (2007). Synthetic affibody molecules: a novel class of affinity ligands for molecular imaging of HER2-expressing malignant tumors. Cancer Res.

Table 1: Biodistribution of radioactivity from [111In]PEP09239 and [111In]ABY-002 in normal NMRI mice.

Organ | Time p.i.
Organ | 1 h | | 4 h | | 24 h
Organ | PEP09239 | ABY-002 | PEP09239 | ABY-002 | PEP09239 | ABY-002
Organ | Uptake of radioactivity (% ID/g)
Blood | 0.39 ± 0.08* | 1.80 ± 0.10 | 0.14 ± 0.03* | 0.64 ± 0.07 | 0.04 ± 0.00 | 0.14 ± 0.00*
Liver | 1.29 ± 0.07* | 2.90 ± 0.10 | 1.10 ± 0.50* | 2.90 ± 0.30 | 1.10 ± 0.30 | 2.43 ± 0.00*
Colon | 0.15 ± 0.06* | 0.60 ± 0.10 | 0.08 ± 0.02* | 0.29 ± 0.06 | 0.07 ± 0.00 | 0.30 ± 0.00*
Kidney | 198 ± 41 | 170 ± 17 | 170 ± 15 | 162 ± 22 | 124 ± 21 | 116 ± 12
Muscle | 0.13 ± 0.04* | 0.40 ± 0.10 | 0.06 ± 0.00* | 0.22 ± 0.02 | 0.05 ± 0.01 | 0.15 ± 0.00*

*P < 0.05, [^111^In]PEP09239 versus [^111^In]ABY-002. For complete data, see Rosik et al. (4).

Abbreviations: NMRI, Naval Medical Research Institute; p.i., postinjection.